# ^111^In-Anti-CD105 MJ7/18 monoclonal antibody

Chemical name: | ^111^In-Anti-CD-105 MJ7/18 monoclonal antibody
Abbreviated name: | ^111^In-MJ7/18 MAb
Synonym: | ^111^In-labeled- anti-endoglin MAb, ^111^In-anti-endoglin MAb, ^111^In-anti-EDG MAb, ^111^In-DTPA-MJ7/18 MAb, ^111^In-anti-TGF-ß binding receptor MAb
Agent Category: | Antibody
Target: | Endoglin (CD105, EDG)
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), Gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4557555), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=10862690) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2022) for more information about CD105

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(111In-anti-endoglin+antibody)+OR+TGF-beta+binding+receptor+endoglin)]

^111^In-Anti-CD105 MJ7/18 monoclonal antibody (^111^In-MJ7/18 MAb), which is formed by the ^111^In conjugation of an intact rat antimouse MJ7/18 MAb against the antigen endoglin (cluster of differentiation 105 (CD105)), an accessory component of the receptor complex of transforming growth factor-β (TGF-β), has been developed for imaging of tumor neovasculature (1). ^111^In is a gamma emitter with a physical t_½_ of 2.8 days.

Because tumor growth and metastasis largely depend on angiogenesis, targeting of tumor vasculature is a promising strategy for cancer imaging and therapy (2). TGF-β is a pleiotropic cytokine that modulates angiogenesis, vascular remodeling, and tumor progression. Three isoforms of TGF-β, β_1_ to β_3_, have been identified. TGF-β_1_ appears to inhibit proliferation and migration of endothelial cells and their ability to form capillaries. CD105 (EDG) is a homodimeric cell membrane glycoprotein of 180 kDa, and it is a component of the TGF-β receptor complex that binds TGF-β_1_ and TGF-β_3_ with high affinity. CD105 is critical for correct blood vessel development. The expression of CD105 on different cells affects cellular response to TGF-β_1_. CD105 is overexpressed in proliferating endothelial cells of tumor vessels, and they prevent TGF-β_1_ inhibition of cellular proliferation (3, 4). Two isoforms of CD105, L and S, have been identified. L-CD105 is a protein of 633 amino acids and is expressed predominantly on endothelial cells. The molecular weight of CD105 is ~180,000 with disulfide-linked subunits of 95,000. The CD105 gene in humans has been mapped to chromosome 9q34→qter.

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (5-7). Quiescent human endothelial cells express CD105 only weakly, but the expression of CD105 is strongly up-regulated on the endothelium of tumor tissues undergoing angiogenesis (4). The high level of expressed CD105 (up to 10^6^ molecules/proliferating cell) appears to be ideal for in vivo imaging and therapy. Tabata et al. (3) first investigated tumor targeting with ^125^I-labeled anti-CD105 MAbs in human breast tumor-bearing severe combined immune deficiency mice. The results showed the possible usefulness of antiangiogenic radioimmunotherapy with radiolabeled anti-CD105 MAbs. Anti-CD105 MAbs labeled with photon emitters can be used for tumor imaging. Fonsatti et al. (1) showed that a ^125^I-labeled anti-CD105 MAb (MAEND3) could efficiently image spontaneous mammary adenocarcinomas in two dogs. ^125^I is not an ideal radionuclide for imaging, but other radioactive iodines with better imaging properties are available. Alternatively, MAb can also be labeled with radiometals. Labeling with radiometals is generally achieved by indirect labeling with use of a bifunctional chelating agent (8, 9). ^111^In is considered one of the radionuclides of choice for antibody imaging studies. Bredow et al. (4) reported the successful preparation of ^111^In-labeled CD105-specific rat antimouse MAb MJ7/18 (IgG_2a_) as a potential molecular angiogenic marker.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(111In-anti-endoglin+antibody)+OR+TGF-beta+binding+receptor+endoglin)]

Bredow et al. (4) obtained CD105-specific rat antimouse MAb MJ7/18 (IgG_2a_) commercially and conjugated the antibody with diethylenetriaminepentaacetic acid (DTPA) cyclic anhydride. A 6-fold molar exces of DTPA cyclic anhydride per mole of antibody was reacted with dialyzed MJ7/18 MAb in borate buffer (pH 8.7) for 4 h (10). Nonreacted DTPA was removed by dialysis at 4 °C against 0.15 mM sodium citrate and 0.15 M sodium chloride (pH 6). ^111^In chloride in 50 mM hydrochloric acid was added to the DTPA-MAb solution and incubated for 1 h at room temperature. ^111^In-MJ7/18 MAb was purified by use of a size-exclusion Sephadex G-25m spin column.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((111In-anti-endoglin+antibody)+OR+TGF-beta+binding+receptor+endoglin)+AND+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((111In-anti-endoglin+antibody)+OR+TGF-beta+binding+receptor+endoglin)+AND+in+vitro)]

Bredow et al. (4) injected 5 μg (≤1.1 MBq (30 μCi)) of ^111^In-MJ7/18 into mice bearing the s.c. CD105-positive B16 melanoma for biodistribution and imaging studies. Immunohistology and autoradiography showed that the MAb bound to the extracellular domain of CD105. ^111^In-MJ7/18 MAb showed intense activity in the tumor periphery where the highest concentrations of vessels were found. Histologic analysis of higher power confirmed that the activity was maximally located on the endothelium of tumor vessels in the periphery of the sections. After i.v. injection of ^111^In-MJ7/18 MAb, radioactivity accumulated in tumors, and ~97% injected dose per g of the blood activity was removed from circulation within 15 min. Based on the single exponential decay model, the blood half-life (t_½_) was <1 min. Radioactivity bound to vascular endothelial cells in tissues of the liver, kidney, and heart. This mouse species showed higher expression of CD105 in these tissues compared with normal human organs. Radioactivity accumulation in percent injected dose per g (% ID/g) in the tumor vasculature (n = 4) occurred rapidly, with 0.75 ± 0.9, 1.69 ± 0.5, 1.67 ± 0.3, and 1.67 ± 0.7 at 2, 15, 60, and 360 min, respectively. In comparison, an ^111^In-nonspecific antibody (R35-95) accumulated slowly but reached the same radioactivity level at 60 min. The ^111^In-MJ7/18 radioactivity levels (% ID/g) of other major organs at 2 min were 2.45 ± 1.3 (blood), 3.17 ± 2.7 (heart), 0.30 ± 0.2 (kidney), 1.93 ± 2.4 (liver), and 2.54 ± 2.6 (lung), The radioactivity levels (% ID/g) at 60 min were 2.39 ± 0.1 (blood), 5.08 ± 1.2 (heart), 6.48 ± 3.8 (kidney), and 16.70 ± 2.6 (liver).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(((111In-anti-endoglin+antibody)+OR+TGF-beta+binding+receptor+endoglin)++AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(111In-anti-endoglin+antibody)+OR+TGF-beta+binding+receptor+endoglin)++AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(((111In-anti-endoglin+antibody)+OR+TGF-beta+binding+receptor+endoglin)++AND+human)]

No publication is currently available.

## References

1 Fonsatti E., Jekunen A.P., Kairemo K.J., Coral S., Snellman M., Nicotra M.R., Natali P.G., Altomonte M., Maio M. (2000). Endoglin is a suitable target for efficient imaging of solid tumors: in vivo evidence in a canine mammary carcinoma model. Clin Cancer Res.
2 Fonsatti E., Altomonte M., Arslan P., Maio M. (2003). Endoglin (CD105): a target for anti-angiogenetic cancer therapy. Curr Drug Targets.
3 Tabata M., Kondo M., Haruta Y., Seon B.K. (1999). Antiangiogenic radioimmunotherapy of human solid tumors in SCID mice using (125)I-labeled anti-endoglin monoclonal antibodies. Int J Cancer.
4 Bredow S., Lewin M., Hofmann B., Marecos E., Weissleder R. (2000). Imaging of tumour neovasculature by targeting the TGF-beta binding receptor endoglin. Eur J Cancer.
5 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
6 Milenic D.E., Brechbiel M.W. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
7 Kowalsky R.J., Falen S.W. (2004). Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. , Washington, D.C.: APhA. 733-752.
8 Fritzberg A.R., Berninger R.W., Hadley S.W., Wester D.W. (1988). Approaches to radiolabeling of antibodies for diagnosis and therapy of cancer. Pharm Res.
9 Hnatowich D.J., Childs R.L., Lanteigne D., Najafi A. (1983). The preparation of DTPA-coupled antibodies radiolabeled with metallic radionuclides: an improved method. J Immunol Methods.
10 Marecos E., Weissleder R., Bogdanov A. (1998). Antibody-mediated versus nontargeted delivery in a human small cell lung carcinoma model. Bioconjug Chem.